# ^111^In-Diethylenetriamine pentaacetic acid-IC2 rat monoclonal autoantibody to pancreatic β-cell surface antigen

Chemical name: | ^111^In-Diethylenetriamine pentaacetic acid-IC2 rat monoclonal autoantibody to pancreatic β-cell surface antigen
Abbreviated name: | ^111^In-DTPA-IC2
Synonym:
Agent category: | Antibody
Target: | Pancreatic β-cell specific antigen
Target category: | Antigen
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IC2%20antibody)]

The β-cell mass (BCM) is a useful indicator of the function of the pancreas. In type I diabetes, β-cells are destroyed, leading to a dramatic decrease in BCM. In type II diabetes, there is a slow and continuous decrease in BCM because of peripheral insulin resistance and increased demand for insulin. Vesicular monoamine transporter (VMAT2) is present in brain monoaminergic neurons and is responsible for collecting neurotransmitters (e.g., dopamine, norepinephrine, and serotonin) from the cytoplasm and storing them in vesicles for synaptic release (1). VMAT2 is also highly expressed by β-cells in the endocrine pancreas but not in the exocrine pancreas. VMAT2 is expressed mainly on the β-cells in the islets of Langerhans and comprises 1%–2% of the pancreatic mass. VMAT2 is a potential target for noninvasive assessment of BCM and pancreatic function. VMAT2 has been studied in vivo with positron emission tomography (PET) using [^11^C]dihydrotetrabenazine (2-hydroxy-3-isobutyl-9-[^11^C]methoxy-10-methoxy-1,2,3,4,6,7-hexahydro-11bH-benzo[a]quinolizine, also known as [^11^C]DTBZ) for the noninvasive study of VMAT2 in the human brain and pancreas. However, a human clinical study showed that the high nonspecific binding in the exocrine pancreas may appear to overestimate BCM on pancreatic [^11^C]DTBZ PET scans (2). Various noninvasive imaging studies of BCM have also been performed (3-5).

Natural autoantibodies are produced when the immune system recognizes one or more of the body's normal constituents as foreign. These autoantibodies attack the body's own cells, tissues, or organs, leading to systemic autoimmune diseases. Brogren et al. (6) prepared a rat monoclonal autoantibody (IC2) with lymphocytes isolated from the spleen and lymph nodes of a spontaneously diabetic BB rat. IC2 is a rat IgM kappa monoclonal antibody. It binds to a sulfatide epitope galactose-3-sulphate on the cell surface of β-cells. The binding of IC2 to β-cells is sensitive to protease treatments. IC2 shows little binding to other rat tissues; however, IC2 exhibits binding to mouse, hamster, and human β-cells (5). The expression of the antigen on the surface of β-cells was found to be dependent on glucose concentrations (7). Kavishwar et al. (8) identified sphingomyelin (SM) patches stabilized by cholesterol on the cell surface of β-cells as targets of IC2. SM has been implicated to play a role in the regulation of insulin synthesis and apoptosis of β-cells (9, 10). Moore et al. (11) performed preliminary studies of ^111^In-diethylenetriamine pentaacetic acid-IC2 (^111^In-DTPA-IC2) in normal mice and mice treated with streptozotocin (STZ) to induce BCM loss and diabetes.

### Related Resource Links:

- Chapters in MICAD (β-cells (http://www.ncbi.nlm.nih.gov/books?term=beta-cell%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (VMAT2 (http://www.ncbi.nlm.nih.gov/gene/6571))
- Articles in Online Mendelian Inheritance in Man (OMIM) (VMAT2 (http://www.ncbi.nlm.nih.gov/omim/193001))
- Clinical trials (VMAT2 (http://www.clinicaltrials.gov/ct2/results?term=VMAT2))
- Drug information in FDA (VMAT2 (http://google2.fda.gov/search?q=VMAT2&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=10))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IC2%20antibody+synthesis)]

Moore et al. (11) reported the radiolabeling of IC2. DTPA-anhydride (4.2 nM) was added to a solution of IC2 (~7 nmol). The mixture was incubated for 4 h at 0°C. Excess DTPA was removed with dialysis. DTPA-IC2 conjugates were mixed with ^111^InCl_3_ in citrate buffer (pH 3). The mixture was incubated for 90 min at room temperature. Excess ^111^In was removed from ^111^In-DTPA-IC2 on spin columns. The radiochemical purity, specific activity, labeling yield, and the number of DTPA molecules per antibody were not reported. ^125^I-IC2 was prepared with Na^125^I using the IodoGen method for ex vivo biodistribution studies.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IC2%20antibody+in+vitro)]

Moore et al. (11) performed in vitro indirect fluorescence staining with IC2 on pancreatic islets isolated from normal mice (n = 10) and human 9L gliosarcoma cells (control). Fluorescence microscopy showed strong fluorescence signals on the cell surface in the core of pancreatic islets but weak or no expression in 9L cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IC2%20antibody+rodentia)]

Ex vivo biodistribution studies were performed in diabetic mice (n = 5, treated with STZ to induce BCM loss and diabetes) and control mice (n = 5) at 24 h after injection of 0.74 MBq (0.02 mCi) ^125^I-IC2 (0.33 nmol) (11). Pancreatic accumulation values were 0.5% injected dose/gram (ID/g) and 0.2% ID/g in the control and diabetic mice (P < 0.005), respectively. The diabetic mice showed ~50% loss of BCM, which was measured with histological staining of pancreas sections. There was a good correlation (r^2^ = 0.936) between radioactivity accumulation and BCM. Histoimmunostaining showed a colocalization of IC2 to insulin-positive β-cells in the islets. Gamma planar imaging sessions of the excised pancreata were performed in normal mice (n = 3) and diabetic mice (n = 3) at 24 h after injection of 0.74 MBq (0.02 mCi) ^111^In-DTPA-IC2 (0.33 nmol). Reduced radioactivity in the pancreata of diabetic mice was observed in comparison to the pancreata of control mice. Radioactivity intensity was correlated with the BCM of a given pancreas. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IC2%20antibody+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IC2%20antibody+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=IC2%20antibody+human)]

No publication is currently available.

## NIH support

R21 DK5811

## References

1 Schuldiner S. (1994). A molecular glimpse of vesicular monoamine transporters. J Neurochem.
2 Goland R., Freeby M., Parsey R., Saisho Y., Kumar D., Simpson N., Hirsch J., Prince M., Maffei A., Mann J.J., Butler P.C., Van Heertum R., Leibel R.L., Ichise M., Harris P.E. (2009). 11C-dihydrotetrabenazine PET of the pancreas in subjects with long-standing type 1 diabetes and in healthy controls. J Nucl Med.
3 Malaisse W.J., Louchami K., Sener A. (2009). Noninvasive imaging of pancreatic beta cells. Nat Rev Endocrinol.
4 Moore A. (2009). Advances in beta-cell imaging. Eur J Radiol.
5 Saudek F., Brogren C.H., Manohar S. (2008). Imaging the Beta-cell mass: why and how. Rev Diabet Stud.
6 Brogren C.H., Hirsch F., Wood P., Druet P., Poussier P. (1986). Production and characterization of a monoclonal islet cell surface autoantibody from the BB rat. Diabetologia.
7 Aaen K., Rygaard J., Josefsen K., Petersen H., Brogren C.H., Horn T., Buschard K. (1990). Dependence of antigen expression on functional state of beta-cells. Diabetes.
8 Kavishwar A., Medarova Z., Moore A. (2011). Unique sphingomyelin patches are targets of a beta-cell-specific antibody. J Lipid Res.
9 Zhang Y., Ranta F., Tang C., Shumilina E., Mahmud H., Foller M., Ullrich S., Haring H.U., Lang F. (2009). Sphingomyelinase dependent apoptosis following treatment of pancreatic beta-cells with amyloid peptides Abeta(1-42) or IAPP. Apoptosis.
10 Kelpe C.L., Moore P.C., Parazzoli S.D., Wicksteed B., Rhodes C.J., Poitout V. (2003). Palmitate inhibition of insulin gene expression is mediated at the transcriptional level via ceramide synthesis. J Biol Chem.
11 Moore A., Bonner-Weir S., Weissleder R. (2001). Noninvasive in vivo measurement of beta-cell mass in mouse model of diabetes. Diabetes.